# 1-^11^C-Methyl-4-piperidinyl n-butyrate

Chemical name: | 1-^11^C-Methyl-4-piperidinyl n-butyrate
Abbreviated name: | ^11^C-MP4B or [^11^C]BMP
Synonym: | [^11^C]nBMP
Agent Category: | Compound
Target: | Butyrylcholinesterase (BChE, BuChE)
Target Category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=butyrylcholinesterase)]

Cholinesterase (ChE) is an enzyme that hydrolyzes the neurotransmitter acetylcholine into choline and acetic acid, and thus shuts off neural transmission (1, 2). There are two types of ChE: acetylcholinesterase (AChE, also known as erythrocyte cholinesterase or acetylcholine acetylhydrolase) and butyrylcholinesterase (BChE or BuChE, also known as plasma cholinesterase, pseudocholinesterase, or acylcholine acylhydrolase). Both enzymes are present in cholinergic and noncholinergic tissues as well as in plasma and other body fluids. They differ in substrate specificity, behavior in excess substrate, and susceptibility to inhibitors (1, 2).

BChE is encoded by the BCHE gene, which is located in humans on chromosome 3q26.1-q26.2 (3). Mutations of the BCHE gene result in various genotypes and phenotypes (4), and some BCHE gene variants, such as atypical, K, J, and H variants, cause reduced activity of BChE. The silent variants lead to total loss of the enzyme activity (0–2% of normal activity). On the other hand, some variants result in increased activity, such as the C5+ variant (combination of BChE with an unidentified protein), the Cynthiana variant (increased amount of BChE than normal level), and the Johannesburg variant (increased BChE activity with normal enzyme level). In the absence of muscle relaxants, there is no known disadvantage for individuals with these variants.

BChE is synthesized in many tissues, including the liver, lungs, heart, and brain. Similar to AChE, a single BCHE gene gives rise to different protein products by alternative splicing in the coding region of the original transcript. This provides a series of diverse but related molecular forms of BChE (G1, G2, and G4). G4 is the predominant isoform in the mature brain. These forms have similar catalytic properties, but they exhibit different cellular and extracellular distributions and non-catalytic activities.

BChE possesses three different enzymatic activities: esterase, aryl acylamidase, and peptidase (1). The esterase activity of BChE plays an important role in scavenging anti-AChE compounds such as cocaine, heroin, and organophosphate before they reach AChE at physiologically important sites. In the absence of AChE, BChE is believed to serve as a backup to AChE in supporting and regulating cholinergic transmission (5). BChE also inactivates some drugs, e.g., aspirin, amitriptyline, and bambuterol (1, 6). The aryl acylamidase activity of BChE may be involved in the crosstalk between serotonergic and cholinergic neurotransmission systems, but it is still poorly understood. The peptidase activity of BChE is related to the development and progress of Alzheimer’s disease (AD) (7, 8), which is characterized by a loss of cholinergic neurons. In the brains of patients with AD, the level of the membrane-bound G4 form of AChE is selectively reduced by 90% or more in certain regions, while the level of the G1 form is largely unchanged. On the contrary, the G1 form of BChE shows a 30–60% increase, while the G4 form decreases or remains the same as in the normal brain. It has been indicated that BChE, which is found in the neuritic plaques and tangles, cleaves the amyloid precursor protein to the β-amyloid protein and helps β-amyloid diffusion to β-amyloid plaques (6). Abnormal expressions of BChE and AChE have also been observed in human tumors such as meningioma, glioma, acoustic neurinomas, and lung, colon, and ovarian cancers (9, 10). However, the relationship between altered BChE and AChE expressions and tumorigenesis is not clear, nor is the efficacy of specific inhibitors as chemotherapeutic agents.

Because of the potential diagnostic and therapeutic values, investigators have synthesized various radiolabeled acetylcholine and butyrylcholine analogs as positron emission tomography (PET) tracers (11-16). These tracers have been used to measure ChE activity, detect diseases with cholinergic deficits, and study the efficacy of ChE inhibitors. N-methylpiperidinyl esters are a group of synthetic AChE substrates; of them, 1-^11^C-methyl-4-piperidinyl acetate (^11^C-MP4A) and 1-^11^C-methyl-4-piperidinyl propionate (^11^C-MP4P) have already been used in the clinic as PET tracers for in vivo assessment of AChE activity associated with AD. 1-^11^C-Methyl-4-piperidinyl n-butyrate (^11^C-MP4B or [^11^C]BMP), a specific radiolabeled substrate of BChE, was developed for in vivo assessment of BChE activity with PET (15-18).

### AChE- and BChE-Related Resource Links

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=acetylcholinesterase++AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (AChE (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=43&log$=genesensor5&logdbfrom=protein) and BChE (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&term=(bche%5bgene%5d)%20AND%20(Homo%20sapiens%5borgn%5d)%20AND%20alive%5bprop%5d%20NOT%20newentry%5bgene%5d&log$=genesensor5&logdbfrom=nuccore&sort=weight)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=cholinesterase)
- Clinical trials (AChE (http://www.clinicaltrials.gov/ct2/results?term=acetylcholinesterase), BChE (http://www.clinicaltrials.gov/ct2/results?term=butyrylcholinesterase))
- Substances (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=cholinesterase) and Compounds (http://www.ncbi.nlm.nih.gov/pccompound/?term=cholinesterase) in PubChem
- Drug information in FDA (http://google-test.fda.gov/search?q=Cholinesterase+inhibitors&x=9&y=10&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=butyrylcholinesterase+and+imaging)]The ^11^C-MP4B was synthesized by the reaction of 4-butyryl-piperidine, generated in situ from its hydrochloride salt using 1,2,2,6,6-pentamethyl-piperidine, and ^11^C-methyl triflate in methanol-acetonitrile for 1 min at 60°C (15-18). The crude product was purified with high-performance liquid chromatography. After addition of sterile propylene glycol-ethanol (7:3 v/v) and HCl, the fraction containing the product was evaporated, re-dissolved in physiological phosphate buffer (0.1 mol/L, pH 7.4), and filtered through a 0.2-µm sterile filter. The radiochemical yield of ^11^C-MP4B was 5–7 GBq (0.135–0.189 Ci) with a 40-min target irradiation with 17-MeV protons at 10 µA. The specific radioactivity was 60 ± 10 GBq/µmol (1.62 ± 0.27 Ci/µmol). The radiochemical purity was >99%, and the tracer was radiochemically stable for more than 90 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=butyrylcholinesterase+and+imaging)]

Snyder et al. analyzed the in vitro enzyme-mediated cleavage rate with purified enzymes of AChE (electric eel) and BChE (horse serum), as well as in whole mouse blood (n = 3 animals) (17). One unit (U) of AChE was defined as the amount of enzyme necessary to hydrolyze 1.0 µmol ACh/min at 25°C and pH 7.4. One U of BChE was similarly defined but was based on the hydrolysis of its specific substrate BCh. Analysis showed that both BCh and MP4B were specific for BChE. The BChE-mediated cleavage rate of MP4B was -0.045 ± 0.002 ΔA/min per U per L (n = 3 assays) at the BChE concentration of 20 U/ml. The AChE-mediated cleavage rates of BCh and MP4B were both well below the accurate detection limit of 0.004 ΔA/min per U per L, even at an enzyme concentration of 100 U/ml. In the whole mouse blood, ^11^C-MP4B was completely metabolized within 30 min at room temperature.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=butyrylcholinesterase+and+imaging)]

Snyder et al. investigated the in vivo distribution in brains of ^11^C-MP4B in female CD-1 mice (n = 28) after tail vein injection (17). ^11^C-MP4B exhibited high initial brain uptake at 1 min after injection. It washed out rapidly with <2% injected dose per gram wet weight (ID/g) trapped in tissues at 30 min after injection. After 30 min, the amount of radioactivity remained constant in all brain regions, indicating complete metabolism of ^11^C-MP4B in both the central nervous system and periphery, and irreversible trapping of the radiolabeled metabolite in brain tissue. The retention fraction in each brain region was calculated as the ratio of radioactivity retained at 30 min to the initial uptake of radioactivity at 1 min after injection. Because studies using [^14^C]methylpiperidinol have shown that the labeled metabolite formed by the peripheral ChE activity is unable to enter the brain, both the retention fraction and the hydrolysis rate constant (k_3_) (see below) depend on complete in vivo metabolism of the radiotracer to form exclusively 1-[^11^C]methyl-4-piperidinol, and these values are indices of the ChE activity in each brain region. The retention fraction of ^11^C-MP4B in mice was 0.11 ± 0.03 for striatum, 0.08 ± 0.02 for cortex, 0.10 ± 0.02 for cerebellum, 0.10 ± 0.02 for hippocampus, and 0.12 ± 0.04 for thalamus, which was consistent with the previous histochemical results of strong BChE reactivity in striatum and thalamic nuclei, and of mild BChE reactivity in neocortex and hippocampus. The detailed data were not provided regarding the identity of the ^11^C-MP4B metabolite and the percentage of the metabolite based on the radioactivity in the tissues.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=AChE)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=butyrylcholinesterase+and+imaging)]

Snyder et al. performed a PET imaging study in a female pigtail monkey (M. nemistrina) after vein injection of ^11^C-MP4B (17). The k_3_ value, which reflects both the actual rate of enzymatic hydrolysis and the local concentration of BChE, was calculated on the basis of the PET data. In contrast to the rodent data, the initial uptake in primate brain was much less. Approximately 50% of the ^11^C-MP4B entering the brain was rapidly metabolized and trapped in brain tissue. The k_3_ values were 0.054 min^-1^ and 0.047 min^-1^ for striatum (caudate and putamen) and cerebral cortex, respectively. This value of k_3_ is in a range in which it can be estimated with good precision and should be sensitive to both increases and decreases in BChE in disease states.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=butyrylcholinesterase+and+imaging)]

Investigators from several groups analyzed the biodistribution of ^11^C-MP4B and its ability to measure the BChE activity with PET in healthy people as well as in patients with AD (15-18).

Roivainen et al. evaluated the distribution and kinetics of ^11^C-MP4B uptake (15). Kinetic analysis (10 patients with AD and 18 healthy controls) showed that the plasma level of intact ^11^C-MP4B decreased rapidly from 28 ± 14% ID at 0.5 min to 7 ± 6% ID at 15 min after injection. The half-life (t_1/2_) in patients with AD and in normal subjects was 1.65 ± 0.73 min and 1.40 ± 0.52 min (P = 0.28), respectively, and the metabolite-corrected t_1/2_ was 5.03 ± 2.19 min and 3.95 ± 1.18 min (P = 0.18), respectively. Large individual variation was observed in the rate of plasma ^11^C-MP4B hydrolysis, but there was no significant difference in the degradation of ^11^C-MP4B either between male and female or between healthy subjects and AD patients (P > 0.05). Approximately 17% of the ^11^C-MP4B radioactivity was bound to human plasma proteins. In the brains of patients with AD, the ^11^C-MP4B exhibited high initial uptake followed by gradual decrease. At ~30 min after injection, the amount of radioactivity reached a plateau in the cerebellum, striatum, and cortex. The highest ^11^C-MP4B activity was detected in the cerebellum, followed by striatum, pons, and thalamus. Lower ^11^C-MP4B activity was seen in cortical areas. Roivainen et al. concluded that ^11^C-MP4B was excreted rapidly through the renal system. The biodistribution of ^11^C-MP4B in the brains of patients with AD appeared to be in accordance with the distribution of BChE observed in postmortem studies of human brains, except for the observed higher activity in striatum than in cortex. However, no comparisons were made between AD patients and control subjects.

Virta et al. analyzed the biodistribution and residence time of ^11^C-MP4B (16). Up to 60% of the injected dose was excreted via the urinary pathway, and the clearance was rapid as 30% of the radioactivity was excreted within 60 min after injection. The organs with the highest radiation-absorbed dose (mGy/MBq) at 2 h after injection in a 70-kg reference man were the urinary bladder (0.019), kidneys (renal cortex, 0.014), liver (0.008), upper large intestine (0.007), trabecular bone (0.005), parotid glands (0.007), and heart wall (0.003). The residence times were 0.113 h for the muscle, 0.068 h for the cortical bone, 0.041 h for the liver, 0.025 h for the urinary bladder content, 0.018 h for the brain, 0.015 h for the red bone marrow, 0.014 h for the kidneys, 0.008 h for the upper large intestine, 0.007 h for the trabecular bone, and 0.006 h for the lung. With a 2-h voiding interval, the effective dose was 4.2 µSv/MBq. The investigators concluded that ^11^C-MP4B caused less radiation burden than previously studied ^11^C-labeled PET tracers. No intolerably high absorbed doses were observed in critical organs. With 740 MBq (20 mCi) of injected radioactivity, the radiation burden was equivalent to 3.11 mSv. This would allow multiple PET examinations per year to be performed on the same subject.

Kuhl et al. investigated and compared the ^11^C-MP4B PET scan data of the brains between healthy control subjects and patients with AD (18). The in vivo k_3_ in control cases agreed well with the regional BChE activity from the biochemical assay of postmortem human brains. BChE activity was 2.5 times lower in cerebral cortex than in cerebellum. The total cerebral cortical k_3_ increased with age, showing 25% higher k_3_ in elderly (62 ± 7 years old; n = 12) than in young (30 ± 9 years old; n = 13) subjects (P = 0.009). Neither sex effect (P = 0.15) nor age by sex interaction (P = 0.17) were significant. Relative to the parietal cortex distribution, the distributions of ^11^C-MP4B in different cerebral cortex regions (frontal, temporal, occipital, visual, posterior cingulate) did not differ significantly (P > 0.1) between young and elderly subjects. Administration of physostigmine (inhibits both BChE and AChE) led to 49 ± 6% inhibition of BChE activity (P = 0.001) as measured with ^11^C-BMP (n = 4 subjects) and 52 ± 9% inhibition of AChE activity (P = 0.0002) as measured with N-[^11^C]methylpiperidin-4-yl propionate ([^11^C]PMP, a substrate of AChE) (n = 5 subjects). The inhibition levels of the two ChEs did not differ significantly (P = 0.6). After treatment with the selective AChE inhibitor donepezil (n = 4 subjects), AChE was significantly inhibited (27 ± 5%, P = 0.003) but BChE was not (4 ± 1.2%, P = 0.5). Comparison between elderly control subjects (n = 12) and AD patients (n = 15) showed that the activities of both AChE (75 ± 13% of normal, P = 0.00001) and BChE activities (82 ± 14% of normal, P = 0.001) were decreased in AD cerebral cortex. Higher BChE/AChE ratio was not observed in AD patients than in control people. The BChE activity also did not increase in human brains after months of selective AChE inhibition. Their findings do not support the concept that BChE-targeted inhibition will benefit patients with AD.

## References

1 Patocka J., Kuca K., Jun D. (2004). Acetylcholinesterase and butyrylcholinesterase--important enzymes of human body. Acta Medica (Hradec Kralove).
2 Chiou S.Y., Huang C.F., Hwang M.T., Lin G. (2009). Comparison of active sites of butyrylcholinesterase and acetylcholinesterase based on inhibition by geometric isomers of benzene-di-N-substituted carbamates. J Biochem Mol Toxicol.
3 Goodall R. (2004). Cholinesterase: phenotyping and genotyping. Ann Clin Biochem.
4 Primo-Parmo S.L., Bartels C.F., Wiersema B., van der Spek A.F., Innis J.W., La Du B.N. (1996). Characterization of 12 silent alleles of the human butyrylcholinesterase (BCHE) gene. Am J Hum Genet.
5 Li B., Duysen E.G., Saunders T.L., Lockridge O. (2006). Production of the butyrylcholinesterase knockout mouse. J Mol Neurosci.
6 Pepeu G., Giovannini M.G. (2009). Cholinesterase inhibitors and beyond. Curr Alzheimer Res.
7 Geula C., Darvesh S. (2004). Butyrylcholinesterase, cholinergic neurotransmission and the pathology of Alzheimer's disease. Drugs Today (Barc).
8 Rao A.A., Sridhar G.R., Das U.N. (2007). Elevated butyrylcholinesterase and acetylcholinesterase may predict the development of type 2 diabetes mellitus and Alzheimer's disease. Med Hypotheses.
9 Soreq H., Zakut H. (1990). Amplification of butyrylcholinesterase and acetylcholinesterase genes in normal and tumor tissues: putative relationship to organophosphorous poisoning. Pharm Res.
10 Montenegro M.F., Ruiz-Espejo F., Campoy F.J., Munoz-Delgado E., de la Cadena M.P., Cabezas-Herrera J., Vidal C.J. (2006). Acetyl- and butyrylcholinesterase activities decrease in human colon adenocarcinoma. J Mol Neurosci.
11 Fukuda H., Okamura N. (2007). Brain Nerve.
12 Kikuchi T., Zhang M.R., Ikota N., Fukushi K., Okamura T., Suzuki K., Arano Y., Irie T. (2004). N-[18F]fluoroethylpiperidin-4-ylmethyl butyrate: a novel radiotracer for quantifying brain butyrylcholinesterase activity by positron emission tomography. Bioorg Med Chem Lett.
13 Johnson N.D., Duysen E.G., Lockridge O. (2009). Intrathecal delivery of fluorescent labeled butyrylcholinesterase to the brains of butyrylcholinesterase knock-out mice: visualization and quantification of enzyme distribution in the brain. Neurotoxicology.
14 Duysen E.G., Lockridge O. (2008). Whole body and tissue imaging of the butyrylcholinesterase knockout mouse injected with near infrared dye labeled butyrylcholinesterase. Chem Biol Interact.
15 Roivainen A., Rinne J., Virta J., Jarvenpaa T., Salomaki S., Yu M., Nagren K. (2004). Biodistribution and blood metabolism of 1-11C-methyl-4-piperidinyl n-butyrate in humans: an imaging agent for in vivo assessment of butyrylcholinesterase activity with PET. J Nucl Med.
16 Virta J.R., Tolvanen T., Nagren K., Bruck A., Roivainen A., Rinne J.O. (2008). 1-11C-methyl-4-piperidinyl-N-butyrate radiation dosimetry in humans by dynamic organ-specific evaluation. J Nucl Med.
17 Snyder S.E., Gunupudi N., Sherman P.S., Butch E.R., Skaddan M.B., Kilbourn M.R., Koeppe R.A., Kuhl D.E. (2001). Radiolabeled cholinesterase substrates: in vitro methods for determining structure-activity relationships and identification of a positron emission tomography radiopharmaceutical for in vivo measurement of butyrylcholinesterase activity. J Cereb Blood Flow Metab.
18 Kuhl D.E., Koeppe R.A., Snyder S.E., Minoshima S., Frey K.A., Kilbourn M.R. (2006). In vivo butyrylcholinesterase activity is not increased in Alzheimer's disease synapses. Ann Neurol.